# 2-(2-(2-(4-((4-(Methylamino)phenyl)ethynyl)phenoxy)ethoxy)[^18^F]fluoroethoxy)ethyl-4-methylbenzenamine

Chemical name: | 2-(2-(2-(4-((4-(Methylamino)phenyl)ethynyl)phenoxy)ethoxy)[^18^F]fluoroethoxy)ethyl-4-methylbenzenamine
Abbreviated name: | [^18^F]AV-138
Synonym:
Agent category: | Compound
Target: | Amyloid-beta peptide
Target category: | Acceptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-138)]

Alzheimer's disease (AD) is a form of dementia with gradual memory loss and progressive decline in mental functions over time (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of β-amyloid peptides consisting of 40–42 amino acids), and intracellular neurofibrillary tangles (filaments of microtubule-binding hyperphosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-Amyloid peptides and tau protein are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for single-photon emission computed tomography and positron emission tomography (PET) (8-13). The binding performance of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Of these analogs, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans and showed more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal/noise ratios for PET imaging because it is highly lipophilic. N-methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1, [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising agent for the imaging of senile plaques in the brain (16). Zhang et al. (17) reported the development of a series of fluorinated polyethylene glycol units (n = 2–5) for PET imaging of β-amyloid plaques in the brain. 2-(2-(2-(4-((4-(Methylamino)phenyl)ethynyl)phenoxy)ethoxy)[^18^F]fluoroethoxy)ethyl-4-methylbenzenamine ([^18^F]AV-138) was validated as a PET imaging agent for β-amyloid plaques in the brain (18).

### Related Resource Links:

- Chapters in MICAD (amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (amyloid (http://www.ncbi.nlm.nih.gov/gene/351))
- Articles in Online Mendelian Inheritance in Man (OMIM) (amyloid (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid))
- Clinical trials (amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in U.S. Food and Drug Administration (amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-138%20and%20synthesis)]

[^18^F]AV-138 was readily synthesized by standard ^18^F-fluorination of the O-tosylated derivative with [^18^F]KF/Kryptofix 2.2.2 for 10 min at 130°C (18). [^18^F]AV-138 was purified with high-performance liquid chromatography. Overall radiochemical yield was 3.3%–8.5%, with a specific activity of >55 GBq/µmol (1.5 Ci/µmol) at the end of synthesis and a radiochemical purity of >98%. Total synthesis time was ~90 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-138%20and%20in%20vitro)]

[^18^F]AV-138 has a binding affinity (K_i_) value of 2.4 ± 0.7 nM for aggregated β-amyloid fibrils (n = 3 postmortem AD brain homogenates) in competition with [^125^I]IMPY (18). The binding signal in AD gray matter homogenates was approximately nine-fold higher than in AD white matter homogenates. [^18^F]AV-138 was bound to the cortex of postmortem AD brain slices but not to control brain slices, as visualized with autoradiography studies. Plaque labeling with [^18^F]AV-138 correlated very well with thioflavin-S fluorescent labeling (r > 0.9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-138%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-138%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-138%20and%20primate%20not%20human)]

PET imaging was performed in the brains of healthy young female rhesus monkeys after injection of [^18^F]AV-138 (19). The radioactivity peaked in the cortex at ~15 min after injection and exhibited slow washout.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AV-138%20and%20humans)]

Carpenter et al. (19) reported PET imaging with [^18^F]AV-138 in a study of 14 AD patients, with 12 healthy, elderly patients as controls. [^18^F]AV-138 binding was quantified with the use of the standardized uptake value ratio (SUVR), which was calculated for the neocortex, with the cerebellum as reference region. Widespread neocortical binding was observed in all AD patients, with a SUVR peak at ~90 min after injection with ~370 MBq (10 mCi) [^18^F]AV-138. A higher neocortical SUVR was observed in AD patients (~2) than in healthy controls (~1) at 90 min. However, the 90 min to reach maximal SUVR is considered to be suboptimal for routine clinical PET imaging. Furthermore, [^18^F]AV-138 exhibits substantial non-cortical (nonspecific) binding.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
16 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
17 Zhang W., Oya S., Kung M.P., Hou C., Maier D.L., Kung H.F. (2005). F-18 Polyethyleneglycol stilbenes as PET imaging agents targeting Abeta aggregates in the brain. Nucl Med Biol.
18 Wey S.P., Weng C.C., Lin K.J., Yao C.H., Yen T.C., Kung H.F., Skovronsky D., Kung M.P. (2009). Validation of an (18)F-labeled biphenylalkyne as a positron emission tomography imaging agent for beta-amyloid plaques. Nucl Med Biol.
19 Carpenter A.P., Pontecorvo M.J., Hefti F.F., Skovronsky D.M. (2009). The use of the exploratory IND in the evaluation and development of 18F-PET radiopharmaceuticals for amyloid imaging in the brain: a review of one company's experience. Q J Nucl Med Mol Imaging.